# ^99m^Tc(CO)_3_-((S-Pyridin-2-ylmethyl)-Cys)-Nle-Asp-His-D-Phe-Arg-Trp-Gly-Lys-NH_2_

[ ^ 99m ^ Tc(CO) _ 3 _ (N,S,N _ Py _ -6)] ^ + ^

Chemical name: | ^99m^Tc(CO)_3_-((S-Pyridin-2-ylmethyl)-Cys)-Nle-Asp-His-D-Phe-Arg-Trp-Gly-Lys-NH_2_
Abbreviated name: | [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^, 7a
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 receptor, MC1R
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide)]

Malignant melanoma is the deadliest form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) (3) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (4). Most cutaneous cell types express MC receptors, proopiomelanocortin (POMC), and prohormone convertases in addition to MCs. However, these receptors have been found to be overexpressed in melanoma cells. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily (5). Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). [^18^F]FDG has been approved (http://www.fda.gov/Drugs/DevelopmentApprovalProcess/Manufacturing/ucm182642.htm) for cancer imaging by the United States Food and Drug Administration. Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (7, 9-12). Jiang et al. (13) prepared a linear α-MSH analog (Cys-Nle-Asp-His-D-Phe-Arg-Trp-Gly-Lys-NH_2_, (NAPamide)) containing a S-pyridin-2-ylmethyl moiety (peptide 6) at the N-terminus Cys for radiolabeling with ^99m^Tc_3_. ^99m^Tc(CO)_3_(S-Pyridin-2-ylmethyl)-Cys)-Nle-Asp-His-D-Phe-Arg-Trp-Gly-Lys-NH_2_ ([^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^) was evaluated in mice bearing melanoma tumors as a potential agent for use with single-photon emission computed tomography (SPECT) imaging to target melanoma.

### Related Resource Links:

- Chapters in MICAD (NAPamide (http://www.ncbi.nlm.nih.gov/books?term=NAPamide%20AND%20micad%5Bbook%5D), MC1R (http://www.ncbi.nlm.nih.gov/books?term=MC1R%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MC1R (http://omim.org/entry/155555))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+and+synthesis)]

Jiang et al. (13) reported the synthesis of [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^. Peptide 6 (N,S,N_Py_-6) was synthesized using standard Fmoc chemistry on an amide resin with an automated peptide synthesizer with 55% yield. Peptide 6 was purified with high-performance liquid chromatography (HPLC). Mass spectroscopy confirmed the molecular weight of the peptide 6 (1,251.4 Da). A solution of 40 nmol peptide 6 and 126 MBq (3.4 mCi) [^99m^Tc(CO)_3_(OH_2_)_3_]^+^ in phosphate-saline buffer (pH 6) was incubated for 30 min at 70°C. [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^ was purified with HPLC. Radiochemical purity (as confirmed with HPLC) was >98%, with a radiochemical yield of >70%. The specific activity was 37.4–70.3 GBq/µmol (1.01–1.90 Ci/µmol). [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^ was >90% intact in mouse serum, or histidine or cysteine solutions at pH 7.4 after 4 h of incubation at 37°C, indicating that the probe was inert to transchelation or degradation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+AND+in+vitro)]

Jiang et al. (13) conducted in vitro competitive receptor-binding studies of fac-[Re(CO)_3_(N,S,N_Py_-6)]^+^ with B16F10 murine melanoma cells for 90 min at 37°C. The radioactive ligand was ^125^I-Tyr^2^-[Nle^4^,D-Phe^7^]α-MSH. The inhibition concentration (IC_50_) was 2.0 ± 0.9 nM. In vitro cellular accumulation studies of [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^ in B16F10 melanoma cells were performed at 4°C or 37°C for 30, 60, and 120 min. [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^ exhibited accumulation in B16F10 cells at 37°C with 1.2 ± 0.08%, 1.7 ± 0.01%, and 2.3 ± 0.08% of incubation dose at 30, 60, and 120 min, respectively. The accumulation was reduced at 4°C with 0.3 ± 0.05%, 0.5 ± 0.08%, and 0.4 ± 0.09% of incubation dose at 30, 60, and 120 min, respectively. Unlabeled NAPamide (α-MSH analog) significantly reduced the accumulation by ~50% at 37°C (P < 0.05) and little inhibition at 4°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+AND+rodentia)]

Jiang et al. (13) performed ex vivo biodistribution studies in nude mice bearing B16F10 murine melanoma tumors. Each mouse received an intravenous injection of 7.4 MBq (200 μCi) [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^. The radioactivity levels in percent injected dose per gram (% ID/g) were obtained at 1 h and 4 h after injection (n = 4 mice per group). The tumor accumulation of radioactivity was 1.20 ± 0.09% ID/g at 1 h and 0.84 ± 0.10% ID/g at 4 h. The organs with the highest accumulation of radioactivity were the kidneys (~7% ID/g) and liver (~4.5% ID/g) at 1 h. The other normal tissues exhibited less accumulation than the tumors at 4 h. The tumor/muscle and tumor/blood ratios at 4 h were 14.1 ± 0.6 and 2.0 ± 0.6, respectively. No blocking studies were performed.

SPECT/CT imaging of mice (n = 4) bearing the B16F10 melanoma was conducted with injection of 7.4 MBq (0.2 mCi) [^99m^Tc(CO)_3_(N,S,N_Py_-6)]^+^ at 1 h (13). The tumor was clearly visualized. Low radioactivity levels were observed in most normal tissues. However, high radioactivity levels were observed in the kidneys, intestines, and liver. Coinjection of excess NAPamide (α-MSH analog) inhibited the tumor accumulation of radioactivity, whereas there was little effect on the accumulation of radioactivity in the normal tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NAPamide+AND+human)]

No publication is currently available.

## NIH Support

P50 CA114747

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 McQuade P., Miao Y., Yoo J., Quinn T.P., Welch M.J., Lewis J.S. (2005). Imaging of melanoma using 64Cu- and 86Y-DOTA-ReCCMSH(Arg11), a cyclized peptide analogue of alpha-MSH. J Med Chem.
4 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
5 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
11 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
12 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
13 Jiang H., Kasten B.B., Liu H., Qi S., Liu Y., Tian M., Barnes C.L., Zhang H., Cheng Z., Benny P.D. (2012). Novel, Cysteine-Modified Chelation Strategy for the Incorporation of [M(I)(CO)(3)](+) (M = Re, (99m)Tc) in an alpha-MSH Peptide. Bioconjug Chem.